# ^99m^Tc-Labeled N^ε49^ mercaptoacetyl derivatives of affibody Z_HER2:342_ targeting the human epidermal growth factor receptor

Chemical name: | ^99m^Tc-Labeled N^ε49^ mercaptoacetyl derivatives of affibody Z_HER2:342_ targeting the human epidermal growth factor receptor
Abbreviated name: | [^99m^Tc]-N^ε49^-maGGG-Z_HER2:342_; [^99m^Tc]-N^ε49^-maSSS-Z_HER2:342_; [^99m^Tc]-N^ε49^-maESE-Z_HER2:342_
Synonym:
Agent Category: | Antibodies
Target: | Human epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure information is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=affibody&cmd=DetailsSearch)]

Overexpression of the epidermal growth factor receptor type 2 (HER2) is a characteristic feature of a variety of cancers, and HER2 levels in tumors (primary or metastatic) are often used to screen for patients who would benefit from anti-HER2 antibody (Ab) therapy (e.g., for breast cancer, etc.), to determine the efficacy of a treatment regimen, or to predict the prognostic outcome for a patient (1). Positron emission tomography or single-photon emission computed tomography (SPECT) imaging with labeled ligands that target HER2 are often used to detect, diagnose, and develop a treatment regimen for cancers that overexpress this receptor in research studies (this is not a Food and Drug Administration approved indication for human as yet) (2). Although many Abs (monoclonal, recombinant, etc.) and their derivatives have been developed and used in the clinical setting for the imaging or radioimmunotherapy of such cancers, these agents have low efficacy because of their immunogenicity, pharmacokinetic properties (long circulating time), and inability to penetrate deep into tissue (due to the large size (~150 kDa)) (3). Consequently, investigators are constantly developing and evaluating new alternatives to the Ab-based imaging agents (3).

Recently, a small (~7 kDa) “Z_HER2:342_ affibody” was engineered (4) and labeled with radionuclides such as ^99m^Tc or ^111^In for the SPECT detection of HER2-overexpressing tumors (2). Later, the affibody and several of its structural derivatives (for details, see Ekblad et al. (5)) were labeled with ^99m^Tc and used for the detection of HER2-expressing cancers under preclinical and clinical conditions (5, 6). In these affibodies, the ^99m^Tc was incorporated into the molecule through a mercaptoacetyl–peptide chelator that was bound to the N-terminus of the peptide structure. Also, it has been shown that close proximity of amino acids to the chelator can influence the stability of the ^99m^Tc chelate (7) and in vivo biodistribution of the imaging agent (5). On basis of these observations, Ekblad et al. investigated the effect of ^99m^Tc chelate positioning in the affibody molecule on the stability and biodistribution of labeled affibodies under in vivo conditions (5). For this, a series of Z_HER2:342_ derivatives with a mercaptoacetate (ma)-peptide chelator placed at the ε amino group of lysine at position 49 (K49), which sits in the middle of the affibody helix 3 structure, were constructed. The Z_HER2:342_ derivatives synthesized and evaluated were ma-glycyl-glycyl-glycyl (N^ε49^-maGGG-Z_HER2:342_), ma-seryl-seryl-seryl (N^ε49^-maSSS-Z_HER2:342_), and ma-glutamyl-seryl-glutamyl (N^ε49^-maESE-Z_HER2:342_). The constructs were respectively labeled with ^99m^Tc, and their stability, in vitro characteristics, and biodistribution in mice bearing xenograft tumors was compared to the corresponding N-terminal placed chelator affibody analogs.

### Other sources of information regarding EGFR

Other EGFR imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad).

Human EGFR ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed.

Human EGFR on OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man).

Human EGFR gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein).

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis and ^99m^Tc labeling of the various affibody derivatives (with the ma-peptide chelator at the N-terminus or the N^ε49^ position) were described by Ekblad et al. (5). The purity of all peptides was >95% as determined with reverse-phase high-performance liquid chromatography and mass spectroscopy. The radiochemical yields of affibodies with the ma-peptide chelator at the N-terminus (^99m^Tc-maGGG-Z_HER2:342_, ^99m^Tc-maSSS-Z_HER2:342_, and ^99m^Tc-maESE-Z_HER2:342_) were 82.0 ± 12.0, 82.3 ± 4.9, and 87.0 ± 8.0%, and the radiochemical yields with the ma-peptide chelator at the N^ε49^ position (^99m^Tc-N^ε49^-maGGG-Z_HER2:342_, ^99m^Tc-N^ε49^-maSSS-Z_HER2:342_, and ^99m^Tc-N^ε49^-maESE-Z_HER2:342_) were 88.5 ± 4.6, 98.5 2.3, and 94.2 ± 3.5%, respectively. Specific activity of the various ^99m^Tc-labeled affibodies was not reported.

Stability of the various radiolabeled affibodies was determined by Ekblad et al. in the presence of 300-fold excess cysteine for 2 h at 37°C (5) as described elsewhere (8). Except for ^99m^Tc-N^ε49^-maGGG-Z_HER2:342_, all other labeled affibody analogs had a stability of 87.5 ± 1.8 to 97.1 ± 0.5% as determined with instant thin-layer chromatography analysis. The stability of ^99m^Tc-N^ε49^-maGGG-Z_HER2:342_ was 58.1 ± 4.7% under these conditions; due to its low stability, this affibody analog was not used for any further studies (5). With the results from this study, the investigators concluded that location of the ma-chelator in the affibody structure could affect the stability of the molecule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342%20in%20vitro%20studies&cmd=DetailsSearch)]

By real-time biospecific interaction analysis, the dissociation constant (K_D)_ values of N^ε49^-maSSS-Z_HER2:342_ and N^ε49^-maESE-Z_HER2:342_ were determined to be similar to their N-terminal analogs, varying between 400 and 500 pM of the ligand (5). Only N^ε49^-maGGG-Z_HER2:342_ had a higher K_D_ (530 pM) than maGGG-Z_HER2:342_ (200 pM).

Using SKOV-3 cells (a human carcinoma–derived cell line expressing high levels of HER2), the antigen binding values of N^ε49^-maSSS-Z_HER2:342_ and N^ε49^-maESE-Z_HER2:342_ were reported to be 21 ± 0.7% and 13.7 ± 1.8%, respectively, compared to 69.3 ± 2.5% and 64.3 ± 2.0%, respectively, for their N-terminal analogs (5). This indicated that placing the ma-peptide chelator complex on the K49 residue influenced the antigen binding properties of the molecules.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342%20rodentia&cmd=DetailsSearch)]

The effect of chelator position and targeting properties of the N-terminus and N^ε49^-labeled affibody peptides was investigated using Balb/c nu/nu mice (n = an average of 4 animals per compound) bearing SKOV-3 cell xenograft tumors (5) as described earlier (8). Determination of radioactivity accumulated in all major organs of the animals showed that, in general, all of the labeled conjugates had a similar pattern of biodistribution in the animals. However, compared to the N-terminal–labeled affibodies, higher amounts of radioactivity from the N^ε49^-labeled affibodies accumulated in the thyroid, stomach, and the salivary glands of the animals (for details, see Supplemental Information for Ekblad et al. (5)). In addition, the tumor uptake of radioactivity derived from ^99m^Tc-N^ε49^-maSSS-Z_HER2:342_ (4.6 ± 0.9% injected radioactivity per gram tissue (% IA/g)) and ^99m^Tc-N^ε49^-maESE-Z_HER2:342_ (2.8% IA/g) was lower than from their corresponding N-terminal analogs (11.5 ± 0.5% IA/g for ^99m^Tc-maSSS-Z_HER2:342_ and 9.0 ± 1.0% IA/g for ^99m^Tc-maESE-Z_HER2:342_). In the kidney, a higher amount of radioactivity accumulated with ^99m^Tc-N^ε49^-maSSS-Z_HER2:342_ (48.6 ± 0.8% IA/g) than with ^99m^Tc-maSSS-Z_HER2:342_ (33.6 ± 1.7% IA/g). Under the same conditions, a lower uptake of label by the kidneys was observed with ^99m^Tc-N^ε49^-maESE-Z_HER2:342_ (17.0 ± 5.0% IA/g) than with ^99m^Tc-maESE-Z_HER2:342_ (34.0 ± 3.6% IA/g). No blocking studies were reported.

From all the studies described above, the investigators concluded that the chelator composition and position of the chelator moiety on the affibody molecule can influence the biodistribution and targeting properties of the affibodies (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342%20Other%20Non%20Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Tolmachev, V., D. Rosik, H. Wallberg, A. Sjoberg, M. Sandstrom, M. Hansson, A. Wennborg, and A. Orlova, Imaging of EGFR expression in murine xenografts using site-specifically labelled anti-EGFR (111)In-DOTA-Z (EGFR:2377) Affibody molecule: aspect of the injected tracer amount. Eur J Nucl Med Mol Imaging, 2009
2 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
3 Holliger P., Hudson P.J. (2005). Engineered antibody fragments and the rise of single domains. Nat Biotechnol.
4 Wahlberg E., Lendel C., Helgstrand M., Allard P., Dincbas-Renqvist V., Hedqvist A., Berglund H., Nygren P.A., Hard T. (2003). An affibody in complex with a target protein: structure and coupled folding. Proc Natl Acad Sci U S A.
5 Ekblad T., Orlova A., Feldwisch J., Wennborg A., Karlstrom A.E., Tolmachev V. (2009). Positioning of 99mTc-chelators influences radiolabeling, stability and biodistribution of Affibody molecules. Bioorg Med Chem Lett.
6 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
7 Qu T., Wang Y., Zhu Z., Rusckowski M., Hnatowich D.J. (2001). Different chelators and different peptides together influence the in vitro and mouse in vivo properties of 99Tcm. Nucl Med Commun.
8 Engfeldt T., Orlova A., Tran T., Bruskin A., Widstrom C., Karlstrom A.E., Tolmachev V. (2007). Imaging of HER2-expressing tumours using a synthetic Affibody molecule containing the 99mTc-chelating mercaptoacetyl-glycyl-glycyl-glycyl (MAG3) sequence. Eur J Nucl Med Mol Imaging.